# ^111^In-Labeled mapatumumab

Chemical name: | ^111^In-Labeled mapatumumab
Abbreviated name: | ^111^In-EC-HGS-ETR1
Synonym:
Agent Category: | Antibody
Target: | Tumor necrosis factor–related apoptosis-inducing ligand receptor 1 (TRAIL-R1)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click here for the nucleotice, protein and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=8743&log$=databasead&logdbfrom=protein#refseq) information regarding TRAIL receptors.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1)]

Although anti-growth factor antibodies (Abs) are available for the treatment of cancers (1-3), another technique under investigation to treat this disease is the use of tumor necrosis factor–related apoptosis-inducing ligand (TRAIL) receptor (TRAIL-R) agonist Abs such as mapatumumab and lexatumumab (4, 5). These antibodies (Abs) activate a complex apoptotic pathway in the tumor cell, thereby inducing cell death. The apoptotic pathway and the four TRAIL-R types in humans (designated 1 through 4) have been described in detail by Johnstone et al. (4) and Ashkenazi (5). Mapatumumab (TRM-1 or HGS-ETR1) is a TRAIL-R1 monoclonal Ab (mAb) that targets TRAIL-R1; it is under commercial development and has been approved for clinical trials (http://clinicaltrials.gov/ct2/results?term=Mapatumumab) by the United States Food and Drug Administration (USFDA) to treat various cancers. A similar mAb, lexatumumab (TRM-2 or HGS-ETR2), is a TRAIL-R2 mAb that acts as an agonist specifically for the TRAIL-R2 and has been approved by the USFDA for clinical trials (http://clinicaltrials.gov/ct2/results?term=lexatumumab).

Paclitaxel and docetaxel are anti-cancer drugs that inhibit the mitosis and proliferation of cells by interfering with the depolymerization of microtubules. The mechanism of action of these drugs was discussed in detail by Saloustros et al. (6). Gong et al. observed that the anti-tumor activity of HGS-ETR1 could be enhanced in mice bearing colorectal cancer cell xenograft tumors with pretreatment with paclitaxel (7). Using HGS-ETR1 labeled with radioactive indium (^111^In) (^111^In-EC-HGS-ETR1), the investigators determined that the activity of HGS-ETR1 was increased because the pretreatment with paclitaxel upregulated the expression of TRAIL-R1 in Colo205 cell xenograft tumors in nude mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis of ^111^In-EC-HGS-ETR1 was described by Gong et al. (7). Briefly, ethylenedicysteine (EC) was coupled to HGS-ETR1 for the chelation of ^111^In using sulfo-N-hydroxysuccinimide (NHS) and 1-ethyl-3-(3-dimethylaminopropyl)carbodiimide hydrochloride (EDC) as the coupling agents. To do this, EC, NHS, and EDC were mixed with HGS-ETR1 and incubated for 17 h at room temperature. The product, EC-HGS-ETR1, was dialyzed (buffer not described) to remove any unbound reagents. The number ofEC per HGS-ETR1, the purification and the yield of EC-HGS-ETR1 were not described by the investigators. Labeling of EC-HGS-ETR1, to obtain ^111^In-EC-HGS-ETR1, was performed by adding [^111^In]-indium chloride to a solution of EC-mAb. The purification and yield of the radiolabeled product were not reported. Although the radiochemical purity of ^111^In-EC-HGS-ETR1 was reported to be >95% (determined with radio thin-layer chromatography), the specific activity of the labeled mAb was not reported.

For use as controls during scintigraphic imaging, ^111^In-EC-bovine serum albumin (BSA) and ^111^In-EC-isotype control mAb were also generated as described above (7).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+in+vitro)]

The steady state levels of TRAIL-R1 and TRAIL-R2 were determined in Colo205 (a human colorectal cancer tumor cell line) and PA-1 (a human ovarian cancer cell line) cells using immunoblots and fluorescence-activated cell sorting (FACS) (7). Both receptor types were expressed in the two cell lines as determined with the immunoblots, but the levels were reported to be higher in the Colo205 cells than in the PA-1 cells. Similar results were obtained with FACS analysis of the two cell lines.

The concentration for 50% inhibition of cell proliferation (IC_50_) for Colo205 cells was determined to be 800 ng/mL and 150 ng/mL for HGS-ETR1 and HGS-ETR2, respectively (7). The PA-1 cells were reported to be resistant to inhibition by both the Abs even at a concentration of 800 ng/mL. This indicated that the number of TRAIL-R1 and -R2 on the PA-1 cell surface was too low to initiate apoptosis on binding of the two respective agonist TRAIL-R mAbs.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+rodentia)]

Gong et al. studied the tumor uptake of ^111^In-EC-HGS-ETR1 in nude mice bearing Colo205 xenograft tumors (7). Imaging studies were performed 12 days after inoculation with the cells when the tumor diameter was ~1 cm. The animals (4 or 5 mice/group) were intravenously (IV) injected with either ^111^In-EC-HGS-ETR1, ^111^In-EC-BSA, or the ^111^In-EC-isotype control mAb, and scintigraphic images were obtained 2, 24, and 48 h later. Using computer-outlined regions of interest, the counts per pixel of the tumor site and the normal muscle were used to obtain the tumor/muscle count density ratios (TM ratio). At 2 h after administration of the radiochemicals, little difference in the TM ratios was noted between the controls and the ^111^In-EC-HGS-ETR1–treated animals. However, at 24 and 48 h after the injection of radioactivity, the TM ratios for the ^111^In-EC-HGS-ETR1 and the labeled control-injected animals were reported to be ~3 and ~2, respectively. No blocking studies were reported and there was no significant difference apparent between the targeted and the control molecules.

In another study, the Colo205 cell xenograft tumor–bearing animals (n = 3 mice) were imaged before and after (at 2 and 24 h after an IV injection of ^111^In-EC-HGS-ETR1) treatment with paclitaxel (7). Animals treated with paclitaxel were imaged 24 h after administration of the drug. When imaging was performed at 2 h after treatment with the labeled mAb, little difference in the TM ratio (~2) was noted in the tumors with or without the paclitaxel treatment. By 24 h the TM ratio was reported to have increased to ~4.2 in tumors of mice treated with paclitaxel compared with a TM ratio of ~2 in the untreated mice. In the same study, PA-1 cell xenograft tumors in animals (n = 3 mice) showed little change in the TM ratio (~1.5) both at 2 and 24 h after the ^111^In-EC-HGS-ETR1 injection. This indicated that very little of the labeled mAb bound to the tumors derived from the PA-1 cells. No blocking studies were reported and the difference between the targeted radioligand and the controls was small. No stastical analysis was reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Chase J.L. (2008). Clinical use of anti-vascular endothelial growth factor monoclonal antibodies in metastatic colorectal cancer. Pharmacotherapy.
2 Patel D.K. (2008). Clinical use of anti-epidermal growth factor receptor monoclonal antibodies in metastatic colorectal cancer. Pharmacotherapy.
3 Sachdev D., Singh R., Fujita-Yamaguchi Y., Yee D. (2006). Down-regulation of insulin receptor by antibodies against the type I insulin-like growth factor receptor: implications for anti-insulin-like growth factor therapy in breast cancer. Cancer Res.
4 Johnstone R.W., Frew A.J., Smyth M.J. (2008). The TRAIL apoptotic pathway in cancer onset, progression and therapy. Nat Rev Cancer.
5 Ashkenazi A. (2008). Directing cancer cells to self-destruct with pro-apoptotic receptor agonists. Nat Rev Drug Discov.
6 Saloustros E., Mavroudis D., Georgoulias V. (2008). Paclitaxel and docetaxel in the treatment of breast cancer. Expert Opin Pharmacother.
7 Gong J., Yang D., Kohanim S., Humphreys R., Broemeling L., Kurzrock R. (2006). Novel in vivo imaging shows up-regulation of death receptors by paclitaxel and correlates with enhanced antitumor effects of receptor agonist antibodies. Mol Cancer Ther.